# ^64^Cu-1,4,7-Triazacyclononane-1,4,7-triacetic acid-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4,7-triacetic acid-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_
Abbreviated name: | ^64^Cu-NOTA-NFB
Synonym: | ^64^Cu-NOTA-TN14003
Agent category: | Peptide
Target: | Chemokine receptor 4 (CXCR4)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NFB)]

Chemokine receptors are G-protein–coupled receptors directing cell movement toward higher concentrations of chemokines. Chemokine receptor 4 (CXCR4) and its ligand, stromal cell–derived factor-1 (SDF-1 or CXCL12), are known to play a major role in the migration of progenitor cells during embryonic development of the central nervous, cardiovascular, and hematopoietic systems (1, 2). In addition, this CXCR4-SDF-1 receptor system has a function in the development, progression, and spread of various cancers (3), and CXCR4 acts as a co-receptor for human immunodeficiency virus (HIV) on CD4^+^ T cells (4). It has been suggested that CXCR4/SDF-1 interaction contributes to the pathogenesis of neurodegenerative and inflammatory conditions (5). CXCR4 is expressed by many different types of cancers, and overexpression of CXCR4 in cancers indicates poor prognosis with aggressive and metastatic tumors and resistance to chemotherapy (6).

CXCR4 is considered to play an important role in HIV infections and cancers. It is critical to perform imaging studies to measure CXCR4 levels under in vivo conditions for various pathological and physiological conditions (7). ^99m^Tc-SDF-1 has been used with single-photon emission computed tomography (SPECT) to determine changes in CXCR4 expression in the heart after a myocardial infarction. ^64^Cu-1,1'-[1,4-Phenylenebis(methylene)]-bis[1,4,8,11-tetraaza-cyclotetradecane] (^64^Cu-AMD3100), an inhibitor of CXCR4 activity, has been studied with positron emission tomography (PET) (8). An ^111^In-labeled CXCR4 antagonist peptide, ^111^In-Ac-TZ14011, has been developed for SPECT imaging of CXCR4 expression in xenograft tumors in mice (9). Tamamura et al. (10) identified TN14003, a 14-amino-acid peptide (Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_) with high anti-HIV and CXCR4 antagonistic activities in vitro. Jacobson et al. (11) radiolabeled TN14003 with 4-[^18^F]fluorobenzoic acid ([^18^F]FBA) to form 4-[^18^F]fluorobenzoyl-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_ (4-[^18^F]F-T140 (http://www.ncbi.nlm.nih.gov/books/NBK53566/#T140-4-18F)) for PET imaging of tumor CXCR4 expression with a high tumor/background ratio. However, 4-[^18^F]F-T140 exhibited high nonspecific accumulation in red blood cells (RBCs), which masked its binding to CXCR4 on tumors. Later, Jacobson et al. (12) replaced 4-fluorobenzoyl in T140 with 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-1,4,7,10-tetraacetic acid (DOTA) to form DOTA-NFB or 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA) to form NOTA-NFB for radiolabeling with ^64^Cu. ^64^Cu-DOTA-NFB and ^64^Cu-NOTA-NFB showed higher tumor/background ratios than 4-[^18^F]F-T140 with lower bindings to RBCs.

### Related Resource Links:

- Chapters in MICAD (CXCR4 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CXCR4+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (CXCR4 (http://www.ncbi.nlm.nih.gov/gene/7852))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CXCR4 (http://www.ncbi.nlm.nih.gov/omim/162643))
- Clinical trials (CXCR4 (http://www.clinicaltrials.gov/ct2/results?term=CXCR4))
- Drug information in FDA (CXCR4 (http://google2.fda.gov/search?q=CXCR4&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NFB%20and%20synthesis)]

Jacobson et al. (12) incubated TN14003 (0.84 µmol) and S-2-(4-isothiocyanatobenzyl)-NOTA (1.01 µmol) in dimethylformamide for 18 h at 4°C. NOTA-NFB was obtained with 50%–62% chemical yield after purification with high-performance liquid chromatography (HPLC). The structure of NOTA-NFB was confirmed with HPLC and mass spectroscopy analysis supporting a 1:1 NOTA to NFB conjugation. Radiolabeling was performed by mixing 370–444 MBq (10–12 mCi) ^64^Cu-acetate with NOTA-NFB (12 nmol) in ammonium acetate buffer at pH 5.5. The mixture was heated for 20 min at 40°C. ^64^Cu-NOTA-NFB was purified with HPLC. The radiochemical purity was 99%, with a specific activity of 37 MBq/nmol (1 mCi/nmol) at the end of purification. The labeling yield was 91 ± 3% (n =5), with a total synthesis time of 50–55 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NFB%20and%20in%20vitro)]

Chinese hamster ovary (CHO) cells were transfected with human CXCR4 (7 × 10^5^ binding sites/cell). A receptor-binding assay was performed with ^125^I-SDF-1. T140 exhibited a 50% inhibition concentration (IC_50_) value of 2.5 nM (11), whereas NOTA-NFB showed a IC_50_ value of 138 nM (12). T140 also exhibited a lower IC_50_ value than NOTA-NFB to inhibit Jurkat T cell migration in response to SDF-1.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NFB%20and%20rodentia)]

Jacobson et al. (12) performed ex vivo biodistribution studies of 1.85 MBq (0.05 mCi) ^64^Cu-NOTA-NFB in nude mice (n = 5) bearing CHO and CHO-CXCR4 tumor xenografts at 4 h after injection. Accumulation in the spleen (CXCR4-expressing organ) was 4.6 ± 0.9% injected dose/gram (ID/g). The blood accumulation was low at <0.5% ID/g. Accumulation in the liver (22% ID/g) and kidneys (20% ID/g) was higher than in the spleen. ^64^Cu-NOTA-NFB exhibited a significantly higher (P > 0.05) accumulation in the CHO-CXCR4 tumors (4.6 ± 0.7% ID/g) than in the CXCR4-negative CHO tumors (~1% ID/g). Co-injection of excess NOTA-NFB (20 nmol) significantly reduced (P < 0.01) the accumulation of radioactivity in the spleen and CXCR4-positive tumors but had little effect in the blood, muscle, and CHO tumors. Some inhibition was observed in the liver, which does not express high levels of CXCR4. On the other hand, the accumulation in the kidneys increased to ~52% ID/g. The tumor/blood and tumor/muscle ratios were 38.9 ± 4.9 and 39.3 ± 2.3, respectively, at 4 h after injection of only ^64^Cu-NOTA-NFB. Co-injection with 20 nmol NOTA-NFB significantly decreased the tumor/blood and tumor/muscle ratios to 12.6 ± 1.9 and 6.1 ± 1.1 (P < 0.01), respectively.

The whole-body distribution of ^64^Cu-NOTA-NFB was assessed with static PET imaging at 1, 2, 4, and 24 h after injection in nude mice (n = 5) bearing CHO and CHO-CXCR4 tumor xenografts (12). The CHO-CXCR4 tumors were clearly visualized along with the abdomen area at 1 h after injection, but the CHO tumors were not. The accumulation in the CHO-CXCR4 tumors was constant over time at ~4% ID/g. There was little radioactivity (<0.5% ID/g) in the blood, muscle, and CHO tumors. The liver showed a higher accumulation of radioactivity than the kidneys (21.2% ID/g versus 15.6% ID/g) at 24 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NFB%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NFB%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NFB%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Juarez J., Bendall L. (2004). SDF-1 and CXCR4 in normal and malignant hematopoiesis. Histol Histopathol.
2 Miller R.J., Banisadr G., Bhattacharyya B.J. (2008). CXCR4 signaling in the regulation of stem cell migration and development. J Neuroimmunol.
3 Rubin J.B. (2009). Chemokine signaling in cancer: one hump or two?. Semin Cancer Biol.
4 Alkhatib G. (2009). The biology of CCR5 and CXCR4. Curr Opin HIV AIDS.
5 Mocchetti I., Bachis A., Masliah E. (2008). Chemokine receptors and neurotrophic factors: potential therapy against aids dementia?. J Neurosci Res.
6 Gelmini S., Mangoni M., Serio M., Romagnani P., Lazzeri E. (2008). The critical role of SDF-1/CXCR4 axis in cancer and cancer stem cells metastasis. J Endocrinol Invest.
7 Misra P., Lebeche D., Ly H., Schwarzkopf M., Diaz G., Hajjar R.J., Schecter A.D., Frangioni J.V. (2008). Quantitation of CXCR4 expression in myocardial infarction using 99mTc-labeled SDF-1alpha. J Nucl Med.
8 Jacobson O., Weiss I.D., Szajek L., Farber J.M., Kiesewetter D.O. (2009). 64Cu-AMD3100--a novel imaging agent for targeting chemokine receptor CXCR4. Bioorg Med Chem.
9 Hanaoka H., Mukai T., Tamamura H., Mori T., Ishino S., Ogawa K., Iida Y., Doi R., Fujii N., Saji H. (2006). Development of a 111In-labeled peptide derivative targeting a chemokine receptor, CXCR4, for imaging tumors. Nucl Med Biol.
10 Tamamura H., Xu Y., Hattori T., Zhang X., Arakaki R., Kanbara K., Omagari A., Otaka A., Ibuka T., Yamamoto N., Nakashima H., Fujii N. (1998). A low-molecular-weight inhibitor against the chemokine receptor CXCR4: a strong anti-HIV peptide T140. Biochem Biophys Res Commun.
11 Jacobson O., Weiss I.D., Kiesewetter D.O., Farber J.M., Chen X. (2010). PET of tumor CXCR4 expression with 4-18F-T140. J Nucl Med.
12 Jacobson, O., I.D. Weiss, L.P. Szajek, G. Niu, Y. Ma, D.O. Kiesewetter, A. Peled, H.S. Eden, J.M. Farber, and X. Chen, Improvement of CXCR4 tracer specificity for PET imaging. J Control Release, 2011